# Radioiodinated anti–TAG-72 CC49 Fab’ antibody fragment

Chemical name: | Radioiodinated anti–TAG-72 CC49 Fab’ antibody fragment
Abbreviated name: | ^125^I-CC49 Fab’
Synonym: | ^125^I-CC49 Ab, ^125^I-CC49
Agent Category: | Fab’ antibody fragment
Target: | (Sialyl-Tn (STn)) TAG-72
Target Category: | Antibody to antigen binding
Method of detection: | Single-photon emission computed tomography (SPECT), planar gamma imaging
Source of signal/contrast: | ^125^I
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=144964805), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=21689921) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=ShowDetailView&TermToSearch=182875&ordinalpos=1&itool=EntrezSystem2.PEntrez.Gene.Gene_ResultsPanel.Gene_RVDocSum) for more information about TAG-72.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(mab+cc49+fragment)+OR+((fab)+2+CC49))]

Radioiodinated anti–TAG-72 CC49 Fab’ antibody fragment (^125^I-CC49 Fab’), which is formed by the conjugation of ^125^I with an anti–tumor-associated glycoprotein 72 (TAG-72) Fab’ antibody fragment, has been developed for gamma imaging of cancers that express TAG-72 (1-3). ^125^I has a relatively long physical half-life (t_½_) of 60 days and a gamma energy that makes it suitable for imaging only in small animals. ^123^I, another radioiodine, has better physical properties for single-photon emission computed tomography (SPECT) and planar gamma imaging in humans.

The TAG-72 antigen was isolated from the LS-174T human colon cancer xenograft as a high molecular weight glycoprotein (molecular mass of 10^3^ kDa) with mucin-like characteristics (4-7). The TAG-72 antigen is expressed on a variety of human adenocarcinomas such as pancreatic, breast, colorectal, prostate, endometrial, and ovarian cancers. This antigen has also been shown to be shed into the serum of cancer patients (8). The murine monoclonal antibody B72.3 (MAb B72.3) against TAG-72 mucin was initially generated by immunization of mice with a membrane-enriched fraction of a human breast carcinoma (9). With the use of affinity-purified TAG-72 from LS-174T as an immunogen, CC49 and other anti–TAG-72 MAbs with higher affinity constants have been produced and characterized (4, 5, 9, 10). CC49 MAb appears to react with a unique disaccharide sialyl-Tn (STn) epitope on TAG-72 (11, 12).

Radiolabeled MAbs have been developed for both the diagnosis and treatment of tumors (13). Radiolabeled B72.3 and CC49 exhibit excellent tumor localization capabilities with potential diagnostic and therapeutic applications in the clinical setting (14, 15). Because of their relatively large size, intact radiolabeled MAbs tend to have unfavorable imaging kinetics, poor tumor penetration, and high potential for human anti-mouse antibody response (10, 16-18). One possible approach to minimize these problems is reducing intact antibodies to smaller antibody fragments such as F(ab’)_2_ and Fab’ (19). Another approach is the development of genetic engineering methods to obtain single-chain Fv constructs (scFv) and multivalent scFv constructs (10, 20, 21). The F(ab’)_2_ and Fab’ fragments can generally be prepared by simple enzymatic cleavage. Pepsin digestion of the intact IgG removes the antibody constant region and produces the F(ab’)_2_ fragment with a molecular weight of 100,000 or the Fab’ fragment with a molecular weight of 50,000 (1). Because of the smaller size, the Fab’ fragment has faster blood clearance and better tumor penetration than intact IgG (2, 22). The removal of the Fc portion during the enzymatic cleavage also reduces nonspecific binding of Fab’ to Fc receptors. The in vitro and in vivo properties of the radioiodinated CC49 Fab’ fragment have been studied (1-3, 23, 24).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(mab+cc49+fragment)+OR+((fab)+2+CC49))+AND+synthesis)]

CC49 MAb IgG was developed by the immunization of mice with a membrane-enriched fraction of a human breast tumor carcinoma or purified TAG-72 (23, 25). CC49 IgG was purified from ascetic fluid obtained from immunized mice. CC49 Fab’ was prepared by pepsin digestion of the purified CC49 IgG (1, 2, 23). Briefly, 10 mg of IgG was first adjusted to 10 mM dithiothreitol in 150 mM Tris-HCl:150 mM NaCl:2 mM EDTA (pH 8.0) and incubated at room temperature for 1 h. The thiol group was blocked using 21–22 mM iodoacetamide at room temperature for 15 min. The IgG was then dialyzed against 100 mM sodium acetate (pH 4.5); 2% pepsin was then added, and the mixture was incubated at 37ºC for 16 h (1, 2, 23). The mixture was adjusted to pH 7.5–8.0, and the Fab’ fragment was separated by molecular sieving. Further purification was performed by ion-exchange chromatography.

Radioiodination of CC49 Fab’ was performed with the use of 1,3,4,6-tetrachloro-3α,6α-diphenylglycoluril (IodoGen) as the oxidizing agent (1, 23). Briefly, CC49 Fab’ in 0.1 M sodium phosphate buffer (pH 7.2) was added to a glass tube coated with 20 μg IodoGen. Approximately 18.5 MBq (0.5 mCi) ^125^I-sodium iodide was added, and the mixture was incubated for 2 min at room temperature. Gel filtration chromatography was performed immediately to remove the unincorporated ^125^I. The specific activity of ^125^I-CC49 Fab’ was 111–185 kBq/μg (3–5 μCi/μg) or 5.55–9.25 MBq/nmol (0.15–0.25 mCi/nmol) on the basis of the molecular weight of 50,000. The labeling efficiency and radiochemical purity were not reported, but the molecular weight and integrity of ^125^I-CC49 Fab’ was confirmed by sodium dodecyl sulfate:polyacrylamide gel electrophoresis. Yokota et al. (3) prepared ^125^I-CC49 Fab’ with a specific activity of 340.4–399.6 kBq/μg (9.2–10.8 μCi/μg) or 17.02–19.98 MBq/nmol (0.46–0.54 mCi/nmol). The radiochemical purity was >90% in this preparation. Yokota et al. (2) also reported a specific activity of 81.4–432.9 kBq/μg (2.2–11.7 μCi/μg) or 4.07–21.83 MBq/nmol (0.11–0.59 mCi/nmol).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=((mab+cc49+fragment)+OR+((fab)+2+CC49)))]

Milenic et al. (1) used different sources of antigen to perform solid-phase radioimmunoassays. The binding percentages of ^125^I-CC49 Fab’ were 5.1%, 11.3%, 8.2%, and 0.3% for purified TAG-72, LS-174T colon carcinoma xenograft, colon carcinoma biopsy, and melanoma xenograft, respectively. The relative affinity constant of ^125^I-CC49 Fab’ was ~2.6 × 10^8^ M^–1^, which was similar to that of intact ^125^I-CC49 IgG (4.3 × 10^8^ M^–1^). In another study, Yokota et al. (2) reported immunoreactivity of 29% for ^125^I-CC49 Fab’ to an extract positive for TAG-72. In comparison, the immunoreactivity of ^125^I-CC49 IgG in this study was 23%.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=((mab+cc49+fragment)+OR+(fab)+2+CC49))+AND+rodentia)]

Biodistribution studies of ^125^I-CC49 Fab’ were performed in nude mice bearing subcutaneous LS-174T human colon carcinomas (0.5–0.8 cm in diameter) on the back (1). Mice were given i.v. injections of 0.28 MBq (7.5 μCi) ^125^I-CC49 Fab’ and then were euthanized at various time points in groups (n = 4−6 mice in each group). The mean tumor radioactivity levels of ^125^I-CC49 Fab’ in percent injected dose per gram (% ID/g) were 6.2 (6 h), 3.7 (24 h), 2.7 (48 h), and 2.0 (72 h) with a standard error of the mean <15%. The mean liver radioactivity levels (% ID/g) were 2.3 (6 h), 0.9 (24 h), 0.4 (48 h), and 0.2 (72 h). The mean kidney radioactivity levels (% ID/g) were 37.0 (6 h), 4.4 (24 h), 0.3 (48 h), and 0.1 (72 h). The tumor/blood radiolocalization indexes (ratios of % ID/g in tumor to % ID/g in normal tissue) were 7.8 (6 h), 48.4 (24 h), 144.2 (48 h), and 242.6 (72 h). In comparison, the tumor/blood radiolocalization indexes for mice injected with ^131^I-CC49 IgG were 0.3 (4 h), 1.6 (24 h), and 4.1 (48 h). A separate pharmacokinetic study (n = 4 mice) showed that ^125^I-CC49 Fab’ had a plasma clearance t_½α_ of 9.1 min and t_½β_ of 88 min, whereas ^131^I-CC49 IgG had a plasma clearance t_½α_ of 39 min and t_½β_ of 113 h. Gamma imaging of a mouse bearing the tumor with a dose of 3.7 MBq (100 μCi) ^131^I-CC49 Fab’ clearly visualized the tumor at 30 h after injection (1).

Yokota et al. (2) conducted microautoradiography studies of ^125^I-CC49 Fab’ (a dose of 4.1 MBq (112 μCi) or 9.6 μg (192 pmol)) in mice bearing LS-174T tumors (0.5–1 cm diameter). The microautoradiography showed that ^125^I-CC49 Fab’ had intermediate tumor penetration in a size-related manner. It provided greater tumor penetration than ^125^I-CC49 IgG during the early time points. This greater penetration decreased after 24 h. In another report, Yokota et al. (3) found that the ^125^I-CC49 Fab’ radioactivity was primarily associated with the cortical tubules in the kidney and Kupffer cells in the liver. In the spleen, the radioactivity was localized to the marginal zone surrounding the lymphoid follicles. The authors suggested that the localization in the liver and spleen in the mice bearing LS-174T tumors was antigen-mediated. In comparison, ^125^I-CC49 IgG radioactivity was found in the renal vasculature and associated with hepatocytes in the liver.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=((mab+cc49+fragment)+OR+(fab)+2+CC49))++AND+(dog+OR+rabbit+OR+pig+OR+sheep))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=((mab+cc49+fragment)+OR+(fab)+2+CC49))+AND+(primate+NOT+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=((mab+cc49+fragment)+OR+(fab)+2+CC49))+AND+human)]

No publication is currently available.

## References

1 Milenic D.E., Yokota T., Filpula D.R., Finkelman M.A., Dodd S.W., Wood J.F., Whitlow M., Snoy P., Schlom J. (1991). Construction, binding properties, metabolism, and tumor targeting of a single-chain Fv derived from the pancarcinoma monoclonal antibody CC49. Cancer Res.
2 Yokota T., Milenic D.E., Whitlow M., Schlom J. (1992). Rapid tumor penetration of a single-chain Fv and comparison with other immunoglobulin forms. Cancer Res.
3 Yokota T., Milenic D.E., Whitlow M., Wood J.F., Hubert S.L., Schlom J. (1993). Microautoradiographic analysis of the normal organ distribution of radioiodinated single-chain Fv and other immunoglobulin forms. Cancer Res.
4 Muraro R., Kuroki M., Wunderlich D., Poole D.J., Colcher D., Thor A., Greiner J.W., Simpson J.F., Molinolo A., Noguchi P., et al. (1988). Generation and characterization of B72.3 second generation monoclonal antibodies reactive with the tumor-associated glycoprotein 72 antigen. Cancer Res.
5 Johnson V.G., Schlom J., Paterson A.J., Bennett J., Magnani J.L., Colcher D. (1986). Analysis of a human tumor-associated glycoprotein (TAG-72) identified by monoclonal antibody B72.3. Cancer Res.
6 Katari R.S., Fernsten P.D., Schlom J. (1990). Characterization of the shed form of the human tumor-associated glycoprotein (TAG-72) from serous effusions of patients with different types of carcinomas. Cancer Res.
7 Xiao J., Horst S., Hinkle G., Cao X., Kocak E., Fang J., Young D., Khazaeli M., Agnese D., Sun D., Martin E. (2005). Pharmacokinetics and clinical evaluation of 125I-radiolabeled humanized CC49 monoclonal antibody (HuCC49deltaC(H)2) in recurrent and metastatic colorectal cancer patients. Cancer Biother Radiopharm.
8 Paterson A.J., Schlom J., Sears H.F., Bennett J., Colcher D. (1986). A radioimmunoassay for the detection of a human tumor-associated glycoprotein (TAG-72) using monoclonal antibody B72.3. Int J Cancer.
9 Colcher D., Hand P.H., Nuti M., Schlom J. (1981). A spectrum of monoclonal antibodies reactive with human mammary tumor cells. Proc Natl Acad Sci U S A.
10 Goel A., Baranowska-Kortylewicz J., Hinrichs S.H., Wisecarver J., Pavlinkova G., Augustine S., Colcher D., Booth B.J., Batra S.K. (2001). 99mTc-labeled divalent and tetravalent CC49 single-chain Fv's: novel imaging agents for rapid in vivo localization of human colon carcinoma. J Nucl Med.
11 Beresford G.W., Pavlinkova G., Booth B.J., Batra S.K., Colcher D. (1999). Binding characteristics and tumor targeting of a covalently linked divalent CC49 single-chain antibody. Int J Cancer.
12 Colcher D., Pavlinkova G., Beresford G., Booth B.J., Batra S.K. (1999). Single-chain antibodies in pancreatic cancer. Ann N Y Acad Sci.
13 Kowalsky R.J., Falen S.W. (2004). and Radiopharmaceuticals in nuclear pharmacy and nuclear medicine, American Pharmacists Association: Washington, D.C. p. 733-752.
14 Colcher D., Minelli M.F., Roselli M., Muraro R., Simpson-Milenic D., Schlom J. (1988). Radioimmunolocalization of human carcinoma xenografts with B72.3 second generation monoclonal antibodies. Cancer Res.
15 Colcher D., Esteban J., Carrasquillo J.A., Sugarbaker P., Reynolds J.C., Bryant G., Larson S.M., Schlom J. (1987). Complementation of intracavitary and intravenous administration of a monoclonal antibody (B72.3) in patients with carcinoma. Cancer Res.
16 Britton K.E. (1990). The development of new radiopharmaceuticals. Eur J Nucl Med.
17 Jain R.K. (1987). Transport of molecules across tumor vasculature. Cancer Metastasis Rev.
18 Primus F.J., Bennett S.J., Kim E.E., DeLand F.H., Zahn M.C., Goldenberg D.M. (1980). Circulating immune complexes in cancer patients receiving goat radiolocalizing antibodies to carcinoembryonic antigen. Cancer Res.
19 Behr T. Becker W. Hannappel E. Goldenberg D.M. Wolf F. Targeting of liver metastases of colorectal cancer with IgG, F(ab')2, and Fab' anti-carcinoembryonic antigen antibodies labeled with 99mTc: the role of metabolism and kinetics Cancer Res 1995 55Suppl23 5777s 5785s 7493346
20 Bird R.E., Hardman K.D., Jacobson J.W., Johnson S., Kaufman B.M., Lee S.M., Lee T., Pope S.H., Riordan G.S., Whitlow M. (1988). Single-chain antigen-binding proteins. Science.
21 Colcher D., Bird R., Roselli M., Hardman K.D., Johnson S., Pope S., Dodd S.W., Pantoliano M.W., Milenic D.E., Schlom J. (1990). In vivo tumor targeting of a recombinant single-chain antigen-binding protein. J Natl Cancer Inst.
22 Goldenberg D.M. (1993). Monoclonal antibodies in cancer detection and therapy. Am J Med.
23 Colcher D., Zalutsky M., Kaplan W., Kufe D., Austin F., Schlom J. (1983). Radiolocalization of human mammary tumors in athymic mice by a monoclonal antibody. Cancer Res.
24 Abergel C., Padlan E.A., Kashmiri S.V., Milenic D., Calvo B., Schlom J. (1993). Crystallographic studies and primary structure of the antitumor monoclonal CC49 Fab'. Proteins.
25 Pavlinkova G., Beresford G.W., Booth B.J., Batra S.K., Colcher D. (1999). Pharmacokinetics and biodistribution of engineered single-chain antibody constructs of MAb CC49 in colon carcinoma xenografts. J Nucl Med.